# 4-[5-(4-[^18^F]Fluoro-phenyl)-[1,3,4]oxadiazol-2-yl]-1,4-diaza-bicyclo[3.2.2]nonane

Chemical name: | 4-[5-(4-[^18^F]Fluoro-phenyl)-[1,3,4]oxadiazol-2-yl]-1,4-diaza-bicyclo[3.2.2]nonane
Abbreviated name: | [^18^F]NS10743
Synonym:
Agent category: | Compound
Target: | Neuronal α7 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system and in peripheral tissues, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (PET) agents for α4β2 nAChR imaging in the brain for studying neuropsychiatric disorders. A-85380 has also been labeled as 5-[^123^I]iodo-A-85380, which has been developed as a single-photon emission computed tomography agent for the non-invasive study of α4β2 nAChR in the brain. On the other hand, there are some implications that homomeric α7 nAChRs play a role in the pathophysiology of neuropsychiatric disorders (6-8). α7 nAChRs are highly expressed in the cerebral cortex, hippocampus, and subcortical limbic regions, which are involved in learning, memory, and information processing (9-11). 4-Bromophenyl-1,4-diazabicyclo(3.2.2)nonane-4-carboxylate (SSR180711) has been shown to be a potent and selective partial agonist for α7 nAChRs with nanomolar affinity (12). 4-[^11^C]Methylphenyl-1,4-diazabicyclo[3.2.2]nonane-4-carboxylate ([^11^C]CHIBA-1001) has been developed as a PET agent for the non-invasive study of α7 nAChR in the brain (13). In this chapter, another α7 nAChR agonist, 4-[5-(4-[^18^F]fluoro-phenyl)-[1,3,4]oxadiazol-2-yl]-1,4-diaza-bicyclo[3.2.2]nonane ([^18^F]NS10743) (14), is being evaluated for use as a PET imaging agent.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nicotinic%20acetylcholine%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (α7 nAChR (http://www.ncbi.nlm.nih.gov/gene/1139))
- Articles in OMIM (α7 nAChR (http://www.ncbi.nlm.nih.gov/omim/118511))
- Clinical trials (α7 nAChR (http://www.clinicaltrials.gov/ct2/results?term=alpha+7+nicotinic+cholinergic+receptors))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743%20and%20synthesis)]

Deuther-Conrad et al. (14) reported the synthesis of [^18^F]NS10743 by nucleophilic substitution of the nitro precursor in the presence of K[^18^F]F/K222 in dimethylformamide. The mixture was allowed to react for 10–15 min at 150°C, and [^18^F]NS10743 was purified with high-performance liquid chromatography (HPLC). The average radiochemical yield was >30% (decay-corrected) at the end of synthesis (EOS). The radiochemical purity was >99% with a specific activity of 150–375 GBq/µmol (4.1–10.1 Ci/µmol) at EOS. Total synthesis time was ~2.5 h from the end of bombardment. LogD_7.2_ (lipophilicity) of [^18^F]NS10743 was determined to be 0.8.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743%20and%20in%20vitro)]

Deuther-Conrad et al. (14) reported that NS10743 exhibited K_i_ values of 11.6 ± 2.6 nM (n = 3) and 84 nM (n = 2) for human α7 nAChR (obtained with the use of [^3^H]methyllycaconitine) and human α3β4 nAChR (obtained with the use of [^3^H]epibatidine), respectively. NS10743 exhibited little affinity for human α4β2 nAChR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743%20and%20rodentia)]

Deuther-Conrad et al. (14) performed ex vivo biodistribution studies in normal mice (n = 4–8/group) at 5, 20, and 60 min after injection of 0.2 MBq (0.0054 mCi) [^18^F]NS10743 (~0.01 nmol). The highest uptake of [^18^F]NS10743 (percentage of injected dose per gram of tissue (% ID/g)) was found in the adrenal (11.3), followed by the liver (11.0), kidneys (9.9), spleen (7.7), stomach (6.5), pancreas (6.0), intestine (4.9), brain (4.8), heart (4.0), muscle (2.5), blood (2.4), and femur (2.4) at 5 min after injection. Most tissues showed lower radioactivity levels at 60 min after injection, with the exceptions of the stomach (10.8) and urinary bladder (79.6). Brain accumulation was 1.7% ID/g at 60 min. HPLC analysis of the plasma showed that 40%–43% of [^18^F]NS10743 was intact at 60 min after injection with one major hydrophilic metabolite. On the other hand, little degradation of [^18^F]NS10743 was detected in the brain and liver (>98% intact) at 60 min and 30 min after injection, respectively. Blocking studies were performed with pretreatment of the selective α7 nAChR agonist SSR180711 (10 mg/kg, 10 min, intraperitoneal) at 60 min after injection. Significant inhibition in radioactivity accumulation was observed in the adrenal (−56%, P < 0.001), brain (−28%, P < 0.004), thymus (−28%, P < 0.012), and pancreas (−21%, P < 0.044). Ex vivo autoradiography of brain sections showed distinct high binding of [^18^F]NS10743 in the hippocampus, thalamus, lateral septal nucleus, and cortical structures. The hippocampus/cerebellum and cortex/cerebellum ratios were 1.7 and 1.5, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NS10743%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Gotti C., Zoli M., Clementi F. (2006). Brain nicotinic acetylcholine receptors: native subtypes and their relevance. Trends Pharmacol Sci.
7 Nomikos G.G., Schilstrom B., Hildebrand B.E., Panagis G., Grenhoff J., Svensson T.H. (2000). Role of alpha7 nicotinic receptors in nicotine dependence and implications for psychiatric illness. Behav Brain Res.
8 Nordberg A. (2001). Nicotinic receptor abnormalities of Alzheimer's disease: therapeutic implications. Biol Psychiatry.
9 Thomsen M.S., Hansen H.H., Timmerman D.B., Mikkelsen J.D. (2010). Cognitive improvement by activation of alpha7 nicotinic acetylcholine receptors: from animal models to human pathophysiology. Curr Pharm Des.
10 Barrantes F.J., Borroni V., Valles S. (2010). Neuronal nicotinic acetylcholine receptor-cholesterol crosstalk in Alzheimer's disease. FEBS Lett.
11 Hajos M., Rogers B.N. (2010). Targeting alpha7 nicotinic acetylcholine receptors in the treatment of schizophrenia. Curr Pharm Des.
12 Biton B., Bergis O.E., Galli F., Nedelec A., Lochead A.W., Jegham S., Godet D., Lanneau C., Santamaria R., Chesney F., Leonardon J., Granger P., Debono M.W., Bohme G.A., Sgard F., Besnard F., Graham D., Coste A., Oblin A., Curet O., Vige X., Voltz C., Rouquier L., Souilhac J., Santucci V., Gueudet C., Francon D., Steinberg R., Griebel G., Oury-Donat F., George P., Avenet P., Scatton B. (2007). SSR180711, a novel selective alpha7 nicotinic receptor partial agonist: (1) binding and functional profile. Neuropsychopharmacology.
13 Hashimoto K., Nishiyama S., Ohba H., Matsuo M., Kobashi T., Takahagi M., Iyo M., Kitashoji T., Tsukada H. (2008). [11C]CHIBA-1001 as a novel PET ligand for alpha7 nicotinic receptors in the brain: a PET study in conscious monkeys. PLoS ONE.
14 Deuther-Conrad W., Fischer S., Hiller A., Nielsen E.O., Timmermann D.B., Steinbach J., Sabri O., Peters D., Brust P. (2009). Molecular imaging of alpha7 nicotinic acetylcholine receptors: design and evaluation of the potent radioligand [18F]NS10743. Eur J Nucl Med Mol Imaging.